# [^18^F]Fluorobenzoyl anti-HER2 Cys-diabody

Chemical name: | [^18^F]Fluorobenzoyl anti-HER2 Cys-diabody
Abbreviated name: | [^18^F]FB-Cys-Db
Synonym:
Agent Category: | Antibodies
Target: | HER2
Target Category: | Receptors
Method of detection: | Positron emission tomography
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | No structure available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=antibody%20fragment%20and%20imaging%20and%20labeling)]

[^18^F]Fluorobenzoyl (FB) anti-HER2 Cys-diabody (Cys-Db), abbreviated as [^18^F]FB-Cys-Db, was synthesized by Olafsen et al. for use in positron emission tomography (PET) of tumors expressing HER2 (1).

Antibodies have long been considered to be the most attractive agents for molecular imaging because of their high specificity and binding affinity (2, 3). However, the usefulness of full antibodies as imaging agents is limited by their long circulation time in blood (several days to weeks), which requires a long time to optimally accumulate in tumors (1–2 days) (2). Because of their large molecular size (150 kDa), antibodies also exhibit poor tumor-penetrating ability, which leads to poor signal/noise ratio. To improve antibody pharmacokinetics without compromising the affinity and specificity, a promising solution is to reduce the antibody size or alter the Fc receptor-binding domain with protein engineering (2, 3). Indeed, various antibody fragments have been generated, such as single-chain variable fragment (scFv; 25–30 kDa), Fab (~50 kDa), and F(ab')_2_ (~110 kDa) fragments, bivalent scFv (tandem scFv and diabody, 50–60 kDa), and scFv-fusion proteins (80 kDa for minibody and 105 kDa for scFv-Fc) (2). These fragments exhibit good tumor penetration, fast clearance kinetics, high affinity, and high tumor/blood ratio, which are desirable for imaging agents. However, several issues with the use of antibody fragments as imaging agents remain to be solved, one of which is the diverse effects of labeling chemistry on the binding affinity of antibody fragments (4, 5).

To reduce the diverse effects of labeling chemistry, various strategies have been designed. For example, Vaidyanathan and Zalutsky prepared ^18^F-labeled antibody fragments using N-succinimidyl-4-[^18^F]fluorobenzoate ([^18^F]SFB), which reacts with the ε-amino group of surface-exposed lysine residues on proteins (6). Labeling with this approach showed no loss of the antibody fragment affinity. Olafsen et al. further improved efficiency and speed of [^18^F]SFB production by adapting the synthesis to a three-step, one-pot, microwave-assisted method, followed by purification using either a single cartridge or high-performance liquid chromatography (HPLC) (1, 6). Alternatively, McCabe et al. first conjugated the diabody to DOTA, followed by ^64^Cu-radiolabeling through DOTA (7). All these strategies have been reported to be efficient and have fewer diverse effects on the binding affinity of antibody fragments. This chapter summarizes the data obtained with [^18^F]FB-Cys-Db. In another chapter, the data obtained with ^64^Cu-DOTA-CysDb are summarized.

### Related Resource Links:

HER2-related imaging agents (http://www.ncbi.nlm.nih.gov/books/?term=HER2+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books) in MICAD

Protein (http://www.ncbi.nlm.nih.gov/protein?term=HER2) and nucleotide (http://www.ncbi.nlm.nih.gov/nuccore?term=HER2) sequences of HER2

Structure (http://www.ncbi.nlm.nih.gov/structure?term=HER2) of HER2

Bioassays (http://www.ncbi.nlm.nih.gov/pcassay?term=HER2) of HER2 in PubChem

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22392499)]

Olafsen et al. synthesized [^18^F]SFB using a facile, one-pot synthesis, which was based on a three-step, microwave-assisted, nonaqueous radiochemical process (1). Microwave heating enables a rapid transformation in each step of the [^18^F]fluorination, deprotection, and activation. Each step was completed within 1–2 min. The total synthesis time for the microwave-assisted, one-pot process was 35–40 min. The decay-corrected RCY of [^18^F]SFB ranged from 17% to 31%, with a radiochemical purity of >95% and specific activity of 7.4–37 GBq/µmol (0.2–1 Ci/μmol) after purification. An improved method of microwave-assisted, one-pot synthesis was later established and resulted in an increased RCY of 35 ± 5%. [^18^F]SFB was stable in phosphate-buffered saline (pH 7.4) for at least 2 h based on radio-HPLC.

Cys-Db labeling with [^18^F]SFB was achieved by incubating the anti-HER2 Cys-Db in sodium borate buffer (pH 8.5) with [^18^F]SFB for 30–45 min at room temperature, followed by HPLC separation (1). The total synthesis time (including [^18^F]SFB synthesis) was ~100 min, and the RCY of [^18^F]FB-Cys-Db was 1.8%–2.5%. The ratio of SFB to Cys-Db in the intact [^18^F]FB-Cys-Db was not reported. Purification with spin column chromatography and HPLC yielded radiochemical purities of 67.9 ± 13.0% (n = 11) and 94.7 ± 4.8% (n = 8), respectively. Although the HPLC method yielded [^18^F]FB-Cys-Db with high radiochemical purity, the investigators concluded that this approach was not practical because it led to significant dilution, requiring concentration of the product prior to injection into the mice (1).

The radiolabeled fraction associated with [^18^F]FB-Cys-Db was determined by measurement of the activity in the bands presented on an SDS-PAGE gel after electrophoresis of an HPLC-purified [^18^F]FB-Cys-Db with a radiochemical purity of 83.7%. Counting revealed that 82.5% of the activity was associated with the band that represented the Cys-Db, and that the remaining radioactivity was associated with higher (3.3%) and lower (14.2%) molecular weight bands.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22392499)]

After binding with MCF-7/HER2 and C6 (HER2-negative) cells for 1 h at room temperature, the immunoreactivity of [^18^F]FB-Cys-Db was determined to be 32.2% (1). The specificity was also demonstrated with competitive cell binding, showing a 75% decrease in binding. When the immunoreactivity was determined with the agents obtained in later improved conjugation reactions, this value was 59.0 ± 10.0% (n = 4) and 52.3 ± 21.9% (n = 5) for the agents purified with spin column chromatography and HPLC, respectively. Less than 1% activity was associated with the C6 control cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/22392499)]

MicroPET images with [^18^F]FB-Cys-Db were obtained from five mice bearing MCF-7/HER2 breast cancer xenografts (1). Two of these mice also carried HER2-negative C6 control tumors. All of the mice were injected with the [^18^F]FB-Cys-Db purified with spin column chromatography. The amount of radioactivity administered ranged from 1.147 to 3.034 MBq (from 31 to 82 μCi).

The MCF-7/HER2 breast cancer xenografts were clearly delineated at 2 h, and the time-activity curves showed retention and a slight increase of activity in the tumor during the first 2 h after injection, whereas a steady decrease was observed in the kidneys and other organs (Table 1). The tumor signal increased further at 4 h and remained strong at 6 h after injection, with the overall background activity reduced. [^18^F]FB-Cys-Db cleared rapidly from the blood during the first 2 h. The half-life times T_1/2α_ and T_1/2β_ calculated from the images were 0.91 min and 58.95 min, respectively.

Low radioactivity was also visible in the HER2-negative C6 tumors, and the radioactivity became invisible at 6 h. Nonspecific background activity, predominantly in the kidneys and bladder, was seen in all animals at 2 h and 6 h after injection. An approximately two-fold increase in positive/negative tumor signal ratio was obtained at 4 h (~1.5:1) and at 6 h (~3:1) after injection. As expected for a rapidly clearing antibody fragment, the ratios of tumor/normal tissues were highest at 6 h in all tissues, except for bladder (Table 1). No blocking studies were reported.

Table 1. Tumor/normal tissue ratios at 4 h and 6 h after injection of [^18^F]FB-Cys-Db.

Ratio | 4 h after injection | 6 h after injection
Tumor/blood | 1.25 | 1.83
Tumor/liver | 2.09 | 3.13
Tumor/kidney | 0.83 | 1.19
Tumor/muscle | 5.50 | 6.87
Tumor/bladder | 0.01 | 0.07

Biodistribution data were obtained from four mice at 6 h after injection. The mean tumor uptake values were 2.87 ± 0.43% injected dose per gram tissue (ID/g) for the positive tumors and ~1% ID/g for the negative tumors. The kidneys had the next highest uptake. The blood and lung had 1%–2% ID/g, whereas uptake values in the liver, spleen, and carcass were all <1% ID/g. The positive tumor uptake was significantly higher (P < 0.05) than the uptakes in all normal organs and negative tumors, with the exception of the kidney (P = 0.3214). No blocking studies were reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term)]

No references are currently available.

## References

1 Olafsen T., Sirk S.J., Olma S., Shen C.K., Wu A.M. (2012). ImmunoPET using engineered antibody fragments: fluorine-18 labeled diabodies for same-day imaging. Tumour Biol.
2 Olafsen T., Wu A.M. (2010). Antibody vectors for imaging. Semin Nucl Med.
3 Kaur S., Venktaraman G., Jain M., Senapati S., Garg P.K., Batra S.K. (2012). Recent trends in antibody-based oncologic imaging. Cancer Lett.
4 Sirk S.J., Olafsen T., Barat B., Bauer K.B., Wu A.M. (2008). Site-specific, thiol-mediated conjugation of fluorescent probes to cysteine-modified diabodies targeting CD20 or HER2. Bioconjug Chem.
5 Shen B.Q., Xu K., Liu L., Raab H., Bhakta S., Kenrick M., Parsons-Reponte K.L., Tien J., Yu S.F., Mai E., Li D., Tibbitts J., Baudys J., Saad O.M., Scales S.J., McDonald P.J., Hass P.E., Eigenbrot C., Nguyen T., Solis W.A., Fuji R.N., Flagella K.M., Patel D., Spencer S.D., Khawli L.A., Ebens A., Wong W.L., Vandlen R., Kaur S., Sliwkowski M.X., Scheller R.H., Polakis P., Junutula J.R. (2012). Conjugation site modulates the in vivo stability and therapeutic activity of antibody-drug conjugates. Nat Biotechnol.
6 Vaidyanathan G. (1992). andZalutsky, M.R. Labeling proteins with fluorine-18 using N-succinimidyl 4-[18F]fluorobenzoate. Int J Rad Appl Instrum B.
7 McCabe K.E., Liu B., Marks J.D., Tomlinson J.S., Wu H., Wu A.M. (2012). An engineered cysteine-modified diabody for imaging activated leukocyte cell adhesion molecule (ALCAM)-positive tumors. Mol Imaging Biol.